# 1-(2-Chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide

Chemical name: | 1-(2-Chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide
Abbreviated name:
Synonym: | [^11^C]PK11195
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195)]

Benzodiazepines, such as diazepam, are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been identified as the central and peripheral benzodiazepine receptors. The central benzodiazepine receptor (CBR) is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the peripheral benzodiazepine receptor (PBR) is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4, 5). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (6-8). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage accompanying several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBR has been studied in vivo by positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([11C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity (9). [^11^C]PK11195 is being developed as a PET agent for the non-invasive study of microglia and macrophage activation in the brain, lung, and heart.

### Related Resource Links:

- Chapters in MICAD (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (PBR (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610))
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))
- Drug information in FDA (PBR (http://google2.fda.gov/search?q=Peripheral-type+benzodiazepine+receptor+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=5&y=5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20synthesis)]

In the report by Hashimoto et al. (10), [^11^C]PK11195 was synthesized by alkylation of the desmethyl precursor with [^11^C]methyl iodide, with subsequent separation by high-performance liquid chromatography. Radiochemical purity was greater than 99%, and total synthesis time was 23 min. The specific activity was 51.8 GBq/μmol (1.4 Ci/μmol) at the end of bombardment. No yield was reported.

Shah et al. (11) described the fully remotely controlled synthesis of [^11^C]S-PK11195 from S-desmethyl-PK11195 and [^11^C]R-PK11195 from R-desmethyl-PK11195 with [^11^C]methyl iodide. The ^11^C-labeled enantiomers were prepared with a reproducible radiochemical yield of 80% (decay-corrected) based on [^11^C]methyl iodide. Total synthesis time was 45 min. Radiochemical purity was >99% with specific activities varying between 20 and 96 GBq/μmol (0.54 and 2.6 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20in%20vitro)]

In vitro autoradiographic studies of [^3^H]PK11195 binding produced K_d_ values of 20.4 ± 1.3, 14.3 ± 2.1, and 3.9 ± 0.4 nM for human high-grade glioma, low-grade glioma, and cortex, respectively (12). The PBR B_max_ values were 12.4 ± 0.7, 4.0 ± 2.0, and 0.79 ± 0.09 pmol/mg protein for human high-grade glioma, low-grade glioma, and cortex, respectively. The high-grade glioma showed a B_max_ 14.5 times higher than that in the cortex. There was also a significant difference between the K_d_ measured in the tumors and that in normal cortex. Le Fur et al. (9) reported that PBR binding sites in rat myocardial membranes were specific and saturable with a K_d_ of 1.4 nM and a B_max_ of 2.25 pmol/mg protein.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20rodentia)]

Biodistribution studies in normal mice showed high accumulation of radioactivity in the adrenal gland (61% injected dose (ID)/g), followed by the lung (32% ID/g), kidney (20% ID/g), heart (20% ID/g), and liver (6% ID/g) at 5 min after injection of [^3^H]PK11195 (10). The level of radioactivity was low (2% ID/g) in the brain and blood. The radioactivity decreased rapidly in the heart, lung, and brain from 5 to 20 min, whereas it increased in the spleen, kidney, and adrenal gland. Coadiministration of unlabeled PK11195 decreased the accumulation in the heart and lung in a dose-dependent manner but had no effect in the blood and brain at 5 min post injection. Almost all of the radioactivity in the heart, lung, and brain was intact [^3^H]PK11195 at 20 min post injection.

Shah et al. (11) investigated the enantiomeric and racemic accumulation of [^11^C]PK11195 in the brains of normal rats and rats with focal cortical lesions (13). They observed no significant differences in the uptakes of the enantiomers in regions lacking PBR binding sites. However, the R-enantiomer was retained to a significantly greater extent than the S-enantiomer in olfactory bulbs/tubercles, which contain some PBR binding sites, as well as in 9-day-old focal cortical lesions, which are greatly enriched in PBR binding sites associated with macrophage infiltration (14). The observed differences are consistent with the approximately 2-fold greater affinity of the R-enantiomer for PBR binding sites reported in vitro (9, 15). Subsequently, most PET studies have used the R-enantiomer.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Charbonneau et al. (16) obtained PET images of the lung and heart in dogs after injection of [^11^C]PK11195. The lung had a higher accumulation than the heart at 1 min post injection, but after 5 min, the radioactivity in the myocardium was higher than in the lung. The radioactivity in the heart remained constant, whereas that in the lung was undetectable at 30 min. The B_max_ for the myocardium was estimated to be 6 nmol/cm^3^. Injection of excess unlabeled PK11195 (568 nmol (0.2 mg)/kg) 30 min after [^11^C]PK11195 (2.2 nmol/kg) led to a rapid decrease (68%) in the radioactivity in the myocardium. Clonazepam (a CBR agonist, 1 mg/kg) and RO 15-1788 (a CBR antagonist, 1 mg/kg) did not inhibit binding of [^11^C]PK11195 to PBRs. On the other hand, diazepam (a peripheral and central agonist, 1 mg/kg) was less effective than PK11195.

Jones et al. (6) assessed the use of R-[^11^C]PK11195 PET to monitor macrophage disposition after particulate challenge to the lung. Repeated PET scanning was performed over 4 weeks after injection of R-[^11^C]PK11195 in rabbits treated with 5-ìm particles of either amorphous (aSiO_2_) or microcrystalline (xSiO_2_) silica implanted in the right upper pulmonary lobes. Implantation of aSiO_2_ led to increased macrophages, few neutrophils, and no fibrosis, whereas xSiO_2_ increased macrophages and neutrophils and caused fibrosis. After both stimuli, radioactivity localized to the challenged area and correlated with macrophage numbers. Radioactivity in challenged/control lung regions peaked at 4 days for aSiO_2_ (2.88; n = 2) and 6 days for xSiO_2_ (4.62; n = 2). The signal remained elevated throughout the study (aSiO_2_, 2.33 ± 0.77, n = 14; xSiO_2_, 3.99 ± 1.29, n = 9), as did macrophage accumulation. Specific binding of R-[^11^C]PK11195 in macrophages was demonstrated by autoradiography in lavage fluid from an inflamed rabbit knee-joint model. These data suggest that PET scanning after [^11^C]PK11195 provides a noninvasive method for the study of macrophage accumulation in the lung.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20%28primate%20not%20human%29)]

Using PET, Petit-Taboue et al. (17) obtained serial brain scans in 3 baboons after injection of [^11^C]PK11195 (37 MBq/kg, or 1 mCi/kg) with or without unlabeled PK11195. The accumulation of radioactivity (0.005-0.008% ID/ml) in the brain peaked at 3-5 min, remained almost constant at this level up to 6-8 min, and then slowly decreased for the final 60 min of study. Both co-injection of and pretreatment (8 min after injection of the tracer) with unlabeled PK11195 (1 mg/kg) initially enhanced the accumulation (0.012-0.030% ID/ml) in the brain, but also markedly enhanced the washout rate compared with controls.

Sette et al. (18) studied the time course of changes, as assessed by PET, in brain uptake in vivo of ^11^C-labeled PK11195 and flumazenil (a CBR antagonist) as indirect and direct markers of neuronal loss, respectively, after focal cerebral ischemia in 10 anesthetized baboons between days 1 and 91 after unilateral middle cerebral artery occlusion. The studies consisted of successive assessments, in the same PET session, of [^11^C]PK11195, [^11^C]flumazenil, cerebral blood flow, and oxygen consumption. Late computed tomographic scans were obtained to map the approximate contours of infarction and to define a concentric peri-infarct area. There was a significant time-dependent increase in [^11^C]PK11195 accumulation in the peri-infarcted area, which reached its maximum at 20 to 40 days after occlusion, presumably attributable to the presence of glial cells/macrophages. In contrast, there was a time- and perfusion-independent significant decrease in [^11^C]flumazenil accumulation in the infarcted area, which remained stable from day 2 onward, representing synaptic damage. Both accumulations were blocked by saturating doses of cold ligands, which confirmed that these changes represented alterations in specific binding.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20human)]

Charbonneau et al. (16) reported on PET studies in 7 healthy male volunteers after injection of 259-777 MBq (7-21 mCi) of [^11^C]PK11195. Accumulation in the lung was high up to 10 min post injection. The radioactivity in the myocardium became detectable at 2 min. The radioactivity in the heart decreased for 20 min and remained constant at 75 min. Injection of excess unlabeled PK11195 (650 nmol/kg) 30 min after [^11^C]PK11195 (0.94 nmol/kg) led to a rapid decrease (48%) in the radioactivity in the myocardium. In a different study (19), formation of plasma metabolites from [^11^C]PK11195 was analyzed in 2 healthy controls and 3 stroke patients. At 5, 20, and 35 min after injection of [^11^C]PK11195 (370 MBq or 1 mCi), 5%, 22% and 32% of the plasma activity, respectively, was attributable to at least two more polar metabolites. However, no metabolites were found in the hearts, lungs, and brains of mice that received injections of [^11^C]PK11195 (10).

[^11^C]PK11195 or R-[^11^C]PK11195 PET has been used mainly for assessing microglia/macrophage activation as an indication of neuronal and tissue damage in various neurodegenerative disorders (such as Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, lateral sclerosis, Huntington’s disease, HIV-associated dementia, and epilepsy), pulmonary diseases, and ischemic stroke [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20%28microglia%20or%20macrophage%29)]. Most of these human studies used a reference tissue (cerebellum or other cortical regions) to measure the accumulation of radioactivity. Kropholler et al. (20) reported that a kinetic plasma (metabolite-corrected) input with a reversible two-tissue compartment model was best for analyzing R-[^11^C]PK11195 kinetics in PET brain studies of 13 human subjects.

Hirvonen et al. (21) performed dynamic whole-body scans after injection of R-[^11^C]PK11195 in five healthy subjects for radiation dosimetry measurement. The mean effective dose was 4.8 µSv/MBq and the highest equivalent organ doses were recorded in the kidneys (14.0 µSv/MBq), spleen (12.5 µSv/MBq) and small intestine (12.2 µSv/MBq).

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 De Souza E.B., Anholt R.R., Murphy K.M., Snyder S.H., Kuhar M.J. (1985). Peripheral-type benzodiazepine receptors in endocrine organs: autoradiographic localization in rat pituitary, adrenal, and testis. Endocrinology.
6 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
7 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
8 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
9 Le Fur G., Vaucher N., Perrier M.L., Flamier A., Benavides J., Renault C., Dubroeucq M.C., Gueremy C., Uzan A. (1983). Differentiation between two ligands for peripheral benzodiazepine binding sites, [3H]RO5-4864 and [3H]PK 11195, by thermodynamic studies. Life Sci.
10 Hashimoto K., Inoue O., Suzuki K., Yamasaki T., Kojima M. (1989). Synthesis and evaluation of 11C-PK 11195 for in vivo study of peripheral-type benzodiazepine receptors using positron emission tomography. Ann Nucl Med.
11 Shah F., Hume S.P., Pike V.W., Ashworth S., McDermott J. (1994). Synthesis of the enantiomers of [N-methyl-11C]PK 11195 and comparison of their behaviours as radioligands for PK binding sites in rats. Nucl Med Biol.
12 Miyazawa N., Hamel E., Diksic M. (1998). Assessment of the peripheral benzodiazepine receptors in human gliomas by two methods. J Neurooncol.
13 Cremer J.E., Hume S.P., Cullen B.M., Myers R., Manjil L.G., Turton D.R., Luthra S.K., Bateman D.M., Pike V.W. (1992). The distribution of radioactivity in brains of rats given [N-methyl-11C]PK 11195 in vivo after induction of a cortical ischaemic lesion. Int J Rad Appl Instrum B.
14 Myers R., Manjil L.G., Cullen B.M., Price G.W., Frackowiak R.S., Cremer J.E. (1991). Macrophage and astrocyte populations in relation to [3H]PK 11195 binding in rat cerebral cortex following a local ischaemic lesion. J Cereb Blood Flow Metab.
15 Dubroeucq M.C., Benavides J., Doble A., Guilloux F., Allam D., Vaucher N., Bertrand P., Gueremy C., Renault C., Uzan A., et al. (1986). Stereoselective inhibition of the binding of [3H]PK 11195 to peripheral-type benzodiazepine binding sites by a quinolinepropanamide derivative. Eur J Pharmacol.
16 Charbonneau P., Syrota A., Crouzel C., Valois J.M., Prenant C., Crouzel M. (1986). Peripheral-type benzodiazepine receptors in the living heart characterized by positron emission tomography. Circulation.
17 Petit-Taboue M.C., Baron J.C., Barre L., Travere J.M., Speckel D., Camsonne R., MacKenzie E.T. (1991). Brain kinetics and specific binding of [11C]PK 11195 to omega 3 sites in baboons: positron emission tomography study. Eur J Pharmacol.
18 Sette G., Baron J.C., Young A.R., Miyazawa H., Tillet I., Barre L., Travere J.M., Derlon J.M., MacKenzie E.T. (1993). In vivo mapping of brain benzodiazepine receptor changes by positron emission tomography after focal ischemia in the anesthetized baboon. Stroke.
19 De Vos F., Dumont F., Santens P., Slegers G., Dierckx R., De Reuck J. (1999). High-performance liquid chromatographic determination of [11C]1-(2-chlorophenyl)-N-methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide in mouse plasma and tissue and in human plasma. J Chromatogr B Biomed Sci Appl.
20 Kropholler M.A., Boellaard R., Schuitemaker A., van Berckel B.N., Luurtsema G., Windhorst A.D., Lammertsma A.A. (2005). Development of a tracer kinetic plasma input model for (R)-[11C]PK11195 brain studies. J Cereb Blood Flow Metab.
21 Hirvonen J., Roivainen A., Virta J., Helin S., Nagren K., Rinne J.O. (2010). Human biodistribution and radiation dosimetry of 11C-(R)-PK11195, the prototypic PET ligand to image inflammation. Eur J Nucl Med Mol Imaging.